# Quinolinium, 1,1'-[1,3-propanediylbis[(dimethyliminio)-3,1-propanediyl]]bis[4-[3-(3-methyl-2(3H)-benzothiazolylidene)-1-propen-1-yl]-,iodide (1:4)

Chemical name: | Quinolinium, 1,1'-[1,3-propanediylbis[(dimethyliminio)-3,1-propanediyl]]bis[4-[3-(3-methyl-2(3H)-benzothiazolylidene)-1-propen-1-yl]-,iodide (1:4) | [image]
Abbreviated name: | TOTO-3 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Nucleic acids (DNA and RNA) | [image]
Target Category: | Nucleic acids | [image]
Method of detection: | Optical imaging | [image]
Source of signal / contrast: | TOTO-3 | [image]
Activation: | Yes | [image]
Studies: | - In vitro; - Rodents | Structures of TO-PRO-3 and TOTO-3 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TOTO-3)]

Quinolinium, 1,1'-[1,3-propanediylbis[(dimethyliminio)-3,1-propanediyl]]bis[4-[3-(3-methyl-2(3H)-benzothiazolylidene)-1-propen-1-yl]-,iodide (1:4), abbreviated as TOTO-3, is a cell-impermeable cyanine acid dye that has a high affinity for nucleic acids (1, 2). TOTO-3 shows weak fluorescence in solution but generates significantly increased quantum yield (100- to 1,000-fold increase) when binding to DNA or RNA (1, 3, 4). Furthermore, TOTO-3 has a relatively long wavelength (maximum excitation/emission, 640/660 nm). These optical properties make it suitable to assess plasma membrane integrity and to detect DNA with optical imaging (2, 5). TOTO-3 is the dimeric form of quinolinium, 4-[3-(3-methyl-2(3H)-benzothiazolylidene)-1-propenyl]-1-[3-(trimethylammonio)propyl]-,diiodide (TO-PRO-3).

To date, chemotherapy remains the treatment of choice for advanced cancer. However, anticancer agents are often much less efficient against tumor cells in vivo compared with their effect in vitro. Several characteristics of tumors cause this inefficiency, such as high interstitial pressure, increased collagen fibers in the extracellular matrix, acidic microenvironment, and cell membrane (2). Ultrasound has been shown to facilitate the penetration of drugs into tumors by several mechanisms, such as ultrasound-induced hyperthermia, which can enhance drug accumulation in tumor tissue and trigger the release of the drug payload from temperature-sensitive carriers, and ultrasound-induced pores in cell membrane, which can improve cell internalization by increasing the membrane permeability (6, 7).

Molecular imaging has been investigated to monitor and quantify the processes of ultrasound-mediated intracellular drug delivery (2). For this purpose, contrast agents have usually been coupled to or loaded into drug carriers. However, coupling contrast agents to small molecules, as with chemotherapeutic drugs, may change their pharmacokinetics and pharmacodynamics (2). An alternative strategy is co-delivery of drug-mimicking contrast agents and small molecule drugs. Deckers et al. tested the feasibility of using a fluorescent nuclear acid staining dye (TOTO-3) as a model drug to monitor ultrasound-mediated delivery in real time (2). In vivo fluorescence imaging demonstrated that an optical contrast agent with characteristics similar to an anti-cancer drug may be used for in vivo monitoring of the drug delivery process in real time (2). This chapter summarizes the data obtained with TOTO-3.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21861287)]

TOTO-3 is commercially available.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21861287)]

Deckers et al. analyzed the cell internalization of TOTO-3 after incubation with mouse rectal carcinoma line CMT-93 cells without or with preliminary permeabilization with 0.2% Tween (2). When cells were permeabilized before incubation with TOTO-3, strong fluorescent staining of the cytoplasmic RNA and nucleoli was observed. On the contrary, the TOTO-3 fluorescence was not detectable in cells without permeabilization, confirming that TOTO-3 is a cell-impermeable dye.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21861287)]

Deckers et al. tested the feasibility of TOTO-3 as a smart probe for in vivo monitoring of ultrasound-mediated intracellular drug delivery (2). RAG 2/g_C mice bearing a CMT-93 tumor on both flanks (n = 8 mice) were first co-injected with TOTO-3 and microbubbles directly into both tumors, and ultrasound (1.5 MHz for 1 min) was then applied to one tumor with the second tumor serving as a control. The time course of ultrasound-mediated intracellular delivery of TOTO-3 was measured with fluorescence imaging. A distinct difference in the fluorescence intensity was observed between the ultrasound-treated and control tumors at 2 h and 4 h after ultrasound application. At these time points, two-fold higher mean signal intensity and an even larger difference in the total and maximum intensities were observed in the ultrasound-treated tumor.

Epifluorescence microscopy was performed on the excised tumor sections to demonstrate the internalization of TOTO-3 (2). Relatively large areas with TOTO-3 signal were observed in the ultrasound-exposed tumor sections. In contrast, control tumor sections typically showed no fluorescence or only single cells with TOTO-3 uptake. The overall signal intensity was quite weak in both cases.

The investigators hypothesized that phagocytic cells, such as macrophages, caused ultrasound-independent uptake of TOTO-3, which may explain the observed fluorescence in the control tumors (2). Anti-CD68 staining revealed a significant presence of macrophages in both control and ultrasound-treated tumors. However, TOTO-3 signal was strongly associated with macrophages only in the control tumors. Ultrasound-independent uptake was further confirmed with isolated intraperitoneal macrophages from female Rag-gamma mice after incubation of TOTO-3 with the macrophages (2). Flow cytometry and confocal microscopy confirmed that macrophages could take up TOTO-3 in an ultrasound-independent manner. The peak fluorescent intensity was in the range of 1 × 10^3^ to 1 × 10^4^, comparable to the intensity observed for the positive control macrophages (permeabilized with 0.2% Tween before incubation with TOTO-3). The negative control sample (incubation without TOTO-3 and Tween) showed negligible fluorescence signal.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Milanovich N., et al. (1996). Binding of TO-PRO-3 and TOTO-3 to DNA: fluorescence and hole-burning studies. Journal of Physical Chemistry.
2 Deckers R., et al. (2011). A fluorescent chromophore TOTO-3 as a 'smart probe' for the assessment of ultrasound-mediated local drug delivery in vivo. Contrast Media Mol Imaging.
3 Martin R.M., Leonhardt H., Cardoso M.C. (2005). DNA labeling in living cells. Cytometry A.
4 Suzuki T., et al. (1997). DNA staining for fluorescence and laser confocal microscopy. J Histochem Cytochem.
5 Zuliani T., et al. (2003). Sensitive and reliable JC-1 and TOTO-3 double staining to assess mitochondrial transmembrane potential and plasma membrane integrity: interest for cell death investigations. Cytometry A.
6 Frenkel V. (2008). Ultrasound mediated delivery of drugs and genes to solid tumors. Adv Drug Deliv Rev.
7 Khaibullina A., et al. (2008). Pulsed high-intensity focused ultrasound enhances uptake of radiolabeled monoclonal antibody to human epidermoid tumor in nude mice. J Nucl Med.